# ^125^I-Labeled mouse anti-human carbonic anhydrase IX monoclonal antibody

Chemical name: | ^125^I-Labeled mouse anti-human carbonic anhydrase IX monoclonal antibody
Abbreviated name: | ^125^I-MAb
Synonym:
Agent Category: | Antibodies
Target: | Carbonic anhydrase IX (CA IX)
Target Category: | Enzymes
Method of detection: | Single-photon emission computed tomography (SPECT) or planar imaging
Source of signal / contrast: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=carbonic%20anhydrase%20IX%20and%20imaging)]

^125^I-Labeled mouse anti-human carbonic anhydrase IX (CA IX) monoclonal antibody (MAb), abbreviated as ^125^I-MAb, is a probe developed by Li et al. for molecular imaging of tumor hypoxia (1).

CA IX is a membrane-associated glycoprotein that consists of an extracellular catalytic domain, a transmembrane anchor, and a short C-terminal cytoplasmic tail (2, 3). The expression of CA IX is largely restricted to the epithelial cells of the gastrointestinal tract, especially the gastric epithelial cells where CA IX catalyzes the hydration of carbon dioxide to bicarbonate and protons (1, 4). CA IX is one of the two CA isoforms (IX and XII) in the CA family that are overexpressed in various solid tumors (3). The CA IX overexpression is closely related to the activation of hypoxia-inducible factor-1 (HIF-1) and the inactivation of the von Hippel-Lindau (VHL) tumor suppressor gene due to hypoxia or the mutation of the VHL gene (5, 6). In this process, HIF-1 upregulates the expression of CA IX while the VHL protein downregulates the expression of CA IX by involving in the degradation of HIF-1 α-subunits. In some renal cell carcinomas, CA IX could be significantly overexpressed (up to 150-fold) because of the VHL mutation and constitutive HIF-1 activation (2, 3, 6).

The direct outcome of CA IX overexpression is the acidification of the tumor microenvironment, leading to extracellular pH values of ~6.5 in contrast to 7.4 in normal tissues (4). The acidic microenvironment has been shown to be associated with tumorigenic transformation, chromosomal rearrangements, extracellular matrix breakdown, and tumor cell migration, invasion, and resistance to radio/chemotherapy (2, 3, 5). CA IX may also play a role in tumor cell growth by providing bicarbonate to the synthesis of pyrimidine nucleotides.

Because of these facts, CA IX has been investigated as a marker for cellular hypoxia and tumor prognosis and as a target for tumor imaging and therapy (7, 8). For these purposes, a large set of chemical inhibitors and several MAb have been developed (7-9). Ahlskog et al. described the generation and characterization of two high-affinity human MAb (A3 and CC7) specific to the extracellular domain of human CA IX (7). The radionuclide-labeled chimeric antibody cG250 and its Fab and F(ab')2 fragments have been tested by Divgi et al. as molecular probes for imaging clear-cell renal carcinomas and HT29 human colorectal tumor xenografts (10). Li et al. investigated the biodistribution of ^125^I-MAb in animals bearing HT29 tumor xenografts (1). The results from these studies suggest that anti-CA IX MAb can selectively recognize CA IX in tumor cells and preferentially localize at sites of hypoxia in tumors after intravenous administration. This chapter summarizes the data obtained with ^125^I-MAb.

### Related Resource Links:

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=carbonic%20anhydrase%209%20%28CA9%29%20and%20Homo%20sapiens) and protein (http://www.ncbi.nlm.nih.gov/protein?term=carbonic%20anhydrase%209%20%28CA9%29%20and%20Homo%20sapiens) sequences of human carbonic anhydrase IX

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=hypoxia-inducible%20factor-1) and protein (http://www.ncbi.nlm.nih.gov/protein?term=hypoxia-inducible%20factor-1) sequences of hypoxia-inducible factor-1 (HIF-1)

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=von%20Hippel-Lindau%20%28VHL%29%20tumor%20suppressor%20gene) and protein (http://www.ncbi.nlm.nih.gov/protein?term=von%20Hippel-Lindau%20%28VHL%29%20tumor%20suppressor%20gene) sequences of von Hippel-Lindau (VHL) tumor suppressor gene

Carbonic anhydrase-targeted clinical trials (http://clinicaltrials.gov/ct2/results?term=carbonic+anhydrase) in clinicaltrials.gov

Articles on carbonic anhydrase IX (http://www.ncbi.nlm.nih.gov/omim?term=carbonic%20anhydrase%209%20%28CA9%29) in Online Mendelian Inheritance in Man

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21968435)]

Mouse anti-human CA IX MAb (the clone information not reported) is commercially available. Li et al. labeled the antibody with no-carrier-added Na^125^I using the Iodogen method (1). The time of labeling reaction was 10 min, and the radiochemical purity of ^125^I-MAb was 98%. ^125^I-MAb was stable in new-born calf serum and phosphate-buffered saline for 96 h without obvious decrease in its radiochemical purity (>90%). The radiochemical yield and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21968435)]

The expression of CA IX in HT-29 tumor xenografts was analyzed with immunohistochemistry of tumor sections, which showed that CA IX was predominantly expressed in the areas adjacent to necrosis but not in the areas of necrosis (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21968435)]

Biodistribution studies were performed in athymic male mice bearing HT-29 xenografts after tail vein injection of 1.295 MBq (35 µCi) ^125^I-MAb (n = 5 mice/time point) (1). During the first 12 h, a relatively high uptake of ^125^I-MAb was observed in the tumors as well as in the liver, kidney, spleen, lung, and intestine. At 24 h, the uptake of ^125^I-MAb in the normal organs decreased, whereas it reached the highest level (4.9 ± 1.2% injected dose per gram tissue (ID/g)) in tumors. The uptake value was significantly higher in tumors than in normal tissues (P < 0.05). However, the highest tumor/muscle ratio (8.16) was observed at 12 h after injection. The uptake in the thyroid was 0.4 ± 0.1% ID/g at 12 h and increased to 1.4 ± 0.04% ID/g at 96 h after injection, indicating metabolic de-iodination of the ^125^I-MAb.

Binding of ^125^I-MAb with whole blood cells in vivo was evaluated at 24 h after injection of 3.7 MBq (100 µCi) ^125^I-MAb (0.1 ml) into an athymic mouse via the tail vein (1). The mouse was euthanized and blood cells were collected and washed completely to remove the unbound ^125^I-MAb. The radioactivity in the blood was higher than in tumors and other organs (see Figure 2 in Li et al. (1)) and this value in the fraction of blood cells was 5.5% of the blood activity at 24 h after injection, indicating that a small fraction of ^125^I-MAb diffused into blood cells.

Planar imaging was performed at 48 h after injection of 5.55 MBq (150 µCi) ^125^I-MAb (0.1 ml) via the tail vein (1). Preferential accumulation of ^125^I-MAb in the tumors was detected. A medium accumulation of radioactivity was also detected in the thyroid. Blocking studies were performed with injection of 100-fold molar excess of unlabeled antibody at 24 h before injection of ^125^I-MAb. The results showed that unlabeled MAb effectively blocked the accumulation of ^125^I-MAb in the tumor. The radioactivity in the thyroid was also decreased significantly, but no explanation for the mechanism of the decrease.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Li J., Shi L., Wang C., Zhang X., Jia L., Li X., Zhou W., Qi Y., Zhang L. (2011). Preliminary biological evaluation of (1)(2)I-labeled anti-carbonic anhydrase IX monoclonal antibody in the mice bearing HT-29 tumors. Nucl Med Commun.
2 Winum J.Y., Rami M., Scozzafava A., Montero J.L., Supuran C. (2008). Carbonic anhydrase IX: a new druggable target for the design of antitumor agents. Med Res Rev.
3 Guler O.O., De Simone G., Supuran C.T. (2010). Drug design studies of the novel antitumor targets carbonic anhydrase IX and XII. Curr Med Chem.
4 Pastorekova S., Zatovicova M., Pastorek J. (2008). Cancer-associated carbonic anhydrases and their inhibition. Curr Pharm Des.
5 Kaluz S., Kaluzova M., Liao S.Y., Lerman M., Stanbridge E.J. (2009). Transcriptional control of the tumor- and hypoxia-marker carbonic anhydrase 9: A one transcription factor (HIF-1) show?. Biochim Biophys Acta.
6 Arjumand W., Sultana S. (2012). Role of VHL gene mutation in human renal cell carcinoma. Tumour Biol.
7 Ahlskog J.K., Schliemann C., Marlind J., Qureshi U., Ammar A., Pedley R.B., Neri D. (2009). Human monoclonal antibodies targeting carbonic anhydrase IX for the molecular imaging of hypoxic regions in solid tumours. Br J Cancer.
8 Stillebroer A.B., Oosterwijk E., Oyen W.J., Mulders P.F., Boerman O.C. (2007). Radiolabeled antibodies in renal cell carcinoma. Cancer Imaging.
9 Rami M., Cecchi A., Montero J.L., Innocenti A., Vullo D., Scozzafava A., Winum J.Y., Supuran C.T. (2008). Carbonic anhydrase inhibitors: design of membrane-impermeant copper(II) complexes of DTPA-, DOTA-, and TETA-tailed sulfonamides targeting the tumor-associated transmembrane isoform IX. ChemMedChem.
10 Divgi C.R., Pandit-Taskar N., Jungbluth A.A., Reuter V.E., Gonen M., Ruan S., Pierre C., Nagel A., Pryma D.A., Humm J., Larson S.M., Old L.J., Russo P. (2007). Preoperative characterisation of clear-cell renal carcinoma using iodine-124-labelled antibody chimeric G250 (124I-cG250) and PET in patients with renal masses: a phase I trial. Lancet Oncol.